# [1-methyl-^11^C]8-Dicyclopropylmethyl-1-methyl-3-propylxanthine

Chemical name: | [1-methyl-^11^C]8-Dicyclopropylmethyl-1-methyl-3-propylxanthine
Abbreviated name: | [^11^C]MPDX
Synonym: | 8-Dicyclopropylmethyl-1-[^11^C]methyl-3-propylxanthine
Agent Category: | Compound
Target: | Adenosine A_1_ receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX)]

Adenosine is an endogenous nucleoside that modulates a number of physiologic functions in the central nervous system (CNS) and in peripheral organs, such as the heart, kidney, and muscle (1, 2). The effect is mediated by two major subtypes of receptors (A_1_ and A_2A_) and two minor subtypes (A_2B_ and A_3_). In the CNS, A_1_ receptors are present both pre- and postsynaptically in the hippocampus, cerebral cortex, thalamus, striatum, and cerebellum. A_2A_ receptors are highly concentrated and colocalized with dopamine D_1_ and D_2_ receptors in the striatum, nucleus accumbens, and olfactory tubercle. A_2A_ receptors are also present in the hippocampus and cortex. A_2B_ receptors are widely distributed, with high concentrations in the gastrointestinal tract. A_3_ receptors are also widely distributed, with high concentrations in the testis. A_1_ and A_3_ receptors mediate inhibition of adenylyl cyclase, whereas A_2A_ and A_2B_ receptors mediate stimulation. Changes in adenosine functions are implicated in epilepsy, ischemic cerebral stroke, movement disorders, sleep disorders, and psychiatric disorders (3-5).

A_1_ receptors have been studied in vivo by positron emission tomography (PET) using [1-methyl-^11^C]8-dicyclopropylmethyl-1-methyl-3-propylxanthine ([^11^C]MPDX), a methyl xanthine analog of KF15372 with selective A_1_ antagonistic activity (6). [^11^C]MPDX is being developed as a PET agent for the non-invasive study of A_1_ receptors in the human brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX%20and%20synthesis)]

In the report by Noguchi et al. (7), [^11^C]MPDX was synthesized by alkylation of the 1-N-desmethyl precursor (8-dicyclopropylmethyl-3-propylxanthine) with [^11^C]methyl iodide in the presence of NaH with subsequent purification by high-performance liquid chromatography (HPLC). Radiochemical purity was greater than 98%. The average specific activity was 49 GBq/μmol (1.3 Ci/μmol) at the end of synthesis. Total synthesis time was 45-60 min.

Kawamura et al. (8) described the synthesis of [^11^C]MPDX from the desmethyl precursor with [^11^C]methyl triflate in the presence of NaOH. This procedure provided an improved radiochemical yield of 34.3% based on [^11^C]methyl triflate. No time of synthesis or specific activity was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX%20and%20in%20vitro)]

The reported K_i_ values of MPDX and KF15372 for the A_1_ receptors were 4.2 nM and 3.0 nM, respectively (7). The K_i_ values for both antagonists for A_2A_ receptors were >100 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX%20and%20rodentia)]

Biodistribution studies in normal mice showed high accumulation of radioactivity in the liver (8.5% of injected dose (ID)/g), followed by the small intestine (3.8% ID/g), pancreas (3.2% ID/g), kidney (2.3% ID/g), and spleen (1.9% ID/g) at 30 min after injection of [^11^C]MPDX (7). The level of radioactivity was low in the brain (0.7% ID/g) and blood (1.5% ID/g). Coadministration of the A_1_ antagonist KF15372, but not A_2A_ antagonist KF17837, decreased the accumulation in the brain in a dose-dependent manner at 15 min post injection. About 22-27% and 62-65% of radioactivity in the plasma and cerebral cortex, respectively, was intact [^11^C]MPDX at 30 min post injection.

Kiyosawa et al. (9) studied the changes in the distribution of central benzodiazepine and presynaptic A_1_ receptors in the superior colliculus (SC) and visual cortex (VC) of rats after monocular enucleation as measured by ex vivo autoradiography. The uptake of [^14^C]deoxyglucose in the SC was decreased by ~40% immediately after enucleation and gradually recovered. The binding of [^11^C]flumazenil to central benzodiazepine receptors in the contralateral SC was increased by 33% at week 2 and then returned to the pre-enucleation levels. The uptake of [^11^C]MPDX by the A_1_ receptors in the contralateral SC decreased by ~67% on day 5 after enucleation and remained depressed thereafter. In the contralateral VC, the uptake of [^14^C]deoxyglucose decreased by ~40% immediately after enucleation followed by a gradual recovery, whereas the accumulation of [^11^C]flumazenil and [^11^C]MPDX was not affected. Axon degeneration decreased the A_1_ receptor density and produced a transient increase of postsynaptic central benzodiazepine receptor density in the enucleated rats as measured by ex vivo autoradiography.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX%20and%20%28dog%20or%20pig%20or%20cat%20or%20sheep%20or%20rabbit%29)]

Shimada et al. (6) obtained PET images of the brain in cats after injection of 199 MBq (5.4 mCi) of [^11^C]MPDX. The regional brain distribution and kinetics of [^11^C]MPDX were studied with magnetic resonance imaging co-registration. The cerebral cortex exhibited the highest accumulation of [^11^C]MPDX (distribution volume (DV) = 4.2 ± 1.7) followed by the striatum (DV = 3.8 ± 1.3), cerebellum (DV = 3.5 ± 1.2), thalamus (DV = 3.1 ± 1.2), midbrain (DV = 2.6 ± 0.9), and whole brain (DV = 2.4 ± 0.8). Co-injection with unlabeled MDPX inhibited binding of [^11^C]MPDX to the regional brain areas.

Nariai et al. (10, 11) studied the adenosine A_1_ receptor with PET using [^11^C]MPDX in a cat cerebral ischemic model (middle cerebral artery occlusion and reperfusion). Eighteen adult cats underwent PET measurement of cerebral blood flow (CBF) with ^15^O-labeled water, A_1_ receptor measurement with [^11^C]MPDX, central benzodiazepine receptor measurement with [^11^C]flumazenil, and glucose metabolism measurement with [^18^F]fluorodeoxyglucose (FDG) after 60 min of occlusion. [^11^C]MPDX binding and [^11^C]flumazenil binding, but not CBF and FDG uptake, were significantly reduced in the groups with more severe ischemic insult than in the groups with no or milder insults. Of the two receptor ligands, the reduction rate of [^11^C]MPDX binding to A_1_ receptors was larger in the group that suffered fatal ischemic insult. Therefore, [^11^C]MPDX PET imaging was suitable for evaluating the function of adenosine A_1_ receptors in relation to cerebral ischemia.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX%20and%20%28primate%20not%20human%29)]

Using PET, Ishiwata et al. (12) obtained serial brain scans in 2 monkeys after injection of 91-141 MBq (2.5-3.8 mCi) of [^11^C]MPDX. Accumulation of radioactivity in the brain peaked at 5 min and then decreased for the final 60 min of study. The fraction of unchanged [^11^C]MPDX in blood samples, as determined by HPLC, was 78%, 70%, 54%, and 41% at 5, 15, 30, and 60 min, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MPDX%20and%20human)]

Kimura et al. (13) reported on PET studies in 7 healthy volunteers after injection of 259-777 MBq (7-21 mCi) of [^11^C]MPDX. In Logan plot analysis, the striatum (0.55) exhibited the highest binding potential ((BP), cerebellum as a reference) for [^11^C]MPDX, followed by the thalamus (0.50), occipital cortex (0.40), parietal cortex (0.33), and temporal cortex (0.28). Fukumitsu et al. (14, 15) extended the human PET studies, using Logan plot analysis with arterial input. The DV was large in the striatum and thalamus, moderate in the cerebral cortices, and small in the cerebellum. The distribution pattern of [^11^C]MPDX in the brain was discretely different from that of CBF as measured by ^15^O-labeled water. At 60 min after injection of [^11^C]MPDX, 75% of plasma radioactivity was from the intact tracer. This percentage was much higher than those in rats (22-27%), cats (6.5%), and monkeys (41%). Naganawa et al. (16) reported that the DV and BP for [^11^C]MPDX in various brain regions could be accurately estimated without arterial blood sampling in 25 subjects. Internal dosimetry data for [^11^C]MPDX in humans are not available in the literature.

## References

1 Fredholm B.B., Abbracchio M.P., Burnstock G., Daly J.W., Harden T.K., Jacobson K.A., Leff P., Williams M. (1994). Nomenclature and classification of purinoceptors. Pharmacol Rev.
2 Palmer T.M., Stiles G.L. (1995). Adenosine receptors. Neuropharmacology.
3 Dunwiddie T.V., Masino S.A. (2001). The role and regulation of adenosine in the central nervous system. Annu Rev Neurosci.
4 El Yacoubi M. Costentin J. Vaugeois J.M. Adenosine A2A receptors and depression Neurology 2003 61Suppl 611 S82 7 14663017
5 von Lubitz D.K. (2001). Adenosine in the treatment of stroke: yes, maybe, or absolutely not?. Expert Opin Investig Drugs.
6 Shimada J., Suzuki F., Nonaka H., Karasawa A., Mizumoto H., Ohno T., Kubo K., Ishii A. (1991). 8-(Dicyclopropylmethyl)-1,3-dipropylxanthine: a potent and selective adenosine A1 antagonist with renal protective and diuretic activities. J Med Chem.
7 Noguchi J., Ishiwata K., Furuta R., Simada J., Kiyosawa M., Ishii S., Endo K., Suzuki F., Senda M. (1997). Evaluation of carbon-11 labeled KF15372 and its ethyl and methyl derivatives as a potential CNS adenosine A1 receptor ligand. Nucl Med Biol.
8 Kawamura K., Ishiwata K. (2004). Improved synthesis of [11C]SA4503, [11C]MPDX and [11C]TMSX by use of [11C]methyl triflate. Ann Nucl Med.
9 Kiyosawa M., Ishiwata K., Noguchi J., Endo K., Wang W.F., Suzuki F., Senda M. (2001). Neuroreceptor bindings and synaptic activity in visual system of monocularly enucleated rat. Jpn J Ophthalmol.
10 Nariai T., Shimada Y., Ishiwata K., Nagaoka T., Shimada J., Kuroiwa T., Ono K., Ohno K., Hirakawa K., Senda M. (2003). PET imaging of adenosine A(1) receptors with (11)C-MPDX as an indicator of severe cerebral ischemic insult. J Nucl Med.
11 Nariai T., Shimada Y., Ishiwata K., Nagaoka T., Shimada J., Kuroiwa T., Ono K.I., Hirakawa K., Senda M., Ohno K. (2003). PET neuroreceptor imaging as predictor of severe cerebral ischemic insult. Acta Neurochir Suppl.
12 Ishiwata K., Nariai T., Kimura Y., Oda K., Kawamura K., Ishii K., Senda M., Wakabayashi S., Shimada J. (2002). Preclinical studies on [11C]MPDX for mapping adenosine A1 receptors by positron emission tomography. Ann Nucl Med.
13 Kimura Y., Ishii K., Fukumitsu N., Oda K., Sasaki T., Kawamura K., Ishiwata K. (2004). Quantitative analysis of adenosine A1 receptors in human brain using positron emission tomography and [1-methyl-11C]8-dicyclopropylmethyl-1-methyl-3-propylxanthine. Nucl Med Biol.
14 Fukumitsu N., Ishii K., Kimura Y., Oda K., Sasaki T., Mori Y., Ishiwata K. (2005). Adenosine A1 receptor mapping of the human brain by PET with 8-dicyclopropylmethyl-1-11C-methyl-3-propylxanthine. J Nucl Med.
15 Fukumitsu N., Ishii K., Kimura Y., Oda K., Sasaki T., Mori Y., Ishiwata K. (2003). Imaging of adenosine A1 receptors in the human brain by positron emission tomography with [11C]MPDX. Ann Nucl Med.
16 Naganawa M., Kimura Y., Nariai T., Ishii K., Oda K., Manabe Y., Chihara K., Ishiwata K. (2005). Omission of serial arterial blood sampling in neuroreceptor imaging with independent component analysis. Neuroimage.